# 2-(2'-((Dimethylamino)methyl)-4'-(3-[^18^F]fluoropropoxy)-phenylthio)benzenamine

Chemical name: | 2-(2'-((Dimethylamino)methyl)-4'-(3-[^18^F]fluoropropoxy)-phenylthio)benzenamine
Abbreviated name: | [^18^F]1, [^18^F]SERT-1
Synonym:
Agent category: | Compound
Target: | Serotonin transporter
Target category: | Transporter
Method of detection: | PET
Source of signal\contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=phenylthio+benzenamine)]

Serotonin (5-hydroxytryptamine, 5-HT) has diverse physiological roles as a neurotransmitter in the central nervous system (1). It is also a regulator of smooth muscle function and platelet aggregation. The brain 5-HT system has been implicated in several neuropsychiatric disorders, including major depression, anxiety, obsessive-compulsive disorder, and schizophrenia (2, 3). The serotonergic transmission is controlled in part by the serotonin transporter (SERT), which regulates the concentration of free, active 5-HT in the synaptic cleft. Citalopram, paroxetine, and fluoxetine were developed as selective SERT inhibitors to treat depression and anxiety disorders by blocking the reuptake of 5-HT [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Citalopram%2C%20paroxetine%20and%20fluoxetine%20%29%20and%20human)]. The blockade led to a higher 5-HT concentration in the synaptic cleft and subsequently to improved patient health.

trans-1,2,3,5,6,10-β-Hexahydro-6-[4-([^11^C]methylthio)phenyl[pyrrolo-[2,1-a]isoquinoline ([^11^C]McN5652) binds selectively to the SERT, and its regional distribution of binding in humans correlates well with the known distribution of the SERT in human brain (4). However, the usefulness of [^11^C]McN5652 is limited by its nonspecific binding and slow release from specific binding sites (5). [^11^C]N,N-Dimethyl-2-(2-amino-4-cyanophenylthio)benzylamine ([^11^C]DASB) was found to be a useful tracer for SERT imaging in animals and humans (6-9). It displayed a nanomolar affinity for SERT and a >1,000-fold affinity for SERT over the dopamine transporter (DAT) and the norepinephrine transporter (NET). Uptake in the SERT-rich brain regions was both saturable and selective for SERT. However, the potential widespread use of [^11^C]DASB is limited by the short half-life of ^11^C (20 min). 2-(2'-((Dimethylamino)methyl)-4'-(3-fluoropropoxy)-phenylthio)benzenamine was shown to be a selective inhibitor of SERT. 2-(2'-((Dimethylamino)methyl)-4'-(3-[^18^F]fluoropropoxy)-phenylthio)benzenamine ([^18^F]1) is being evaluated as a useful tool for SERT imaging.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=phenylthio+benzenamine%20AND%20synthesis%5BAll%20Fields%5D)]

[^18^F]1 was synthesized by nucleophilic [^18^F]fluorination of its O-mesylated precursor in acetonitrile solution of K_2_CO_3_/Kryptofix222 for 3 min at 100ºC (10, 11). [^18^F]1 was purified with high-performance liquid chromatography with radiochemical yields of 10–35% (decay-corrected) in a total synthesis time of ~60 min. The specific activity was 11.84–251.6 GBq/μmol (0.32–6.8 Ci/μmol) at the end of synthesis with radiochemical purities of >97%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=phenylthio+benzenamine%20AND%20in%20vitro)]

The transporter-binding affinity of 2-(2'-((dimethylamino)methyl)-4'-(3-fluoropropoxy)-phenylthio)benzenamine was evaluated with competitive radioaffinity assays for SERT, norepinephrine (NET), and dopamine (DAT) transporters using stably transfected cell lines (11). Binding affinity (K_i_, nM) at SERT, NET, and DAT were 0.27, 11.9, and 299 nM, respectively. Selective binding of 2-(2'-((dimethylamino)methyl)-4'-(3-fluoropropoxy)-phenylthio)benzenamine to SERT over NET was also measured using rat cortical membranes with K_i_ values of 0.24 and 12.4 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=phenylthio+benzenamine%20AND%20%28%22rodentia%22%5BMeSH%20Terms%5D%20OR%20rodentia%5BText%20Word%5D%29)]

Wang et al. (10) performed biodistribution studies in normal rats (n = 3 rats/group). Intravenous injection of [^18^F]1 in rats resulted in high uptake of radioactivity in the lungs (3.86% injected dose (ID)/g) and kidneys (3.93% ID/g) at 30 min after injection; less pronounced uptake was seen in the whole brain (1.23% ID/g). Uptake in the thalamus (0.64% ID/g), hippocampus (0.79% ID/g), striatum (0.90% ID/g), cortex (1.00% ID/g), and hypothalamus (1.22% ID/g) was higher than the cerebellum (0.35% ID/g) at 30 min. The brain region radioactivity was >75% blocked with pretreatment of IDAM (SERT inhibitor) except in the cerebellum, which indicates that SERT is low in the cerebellum and the cerebellum can be used as a reference region. Pretreatment with DAT inhibitor GBR12909 did not inhibit the regional accumulation, and pretreatment with NET inhibitor nisoxetine showed only marginal inhibition. Radioactivity cleared gradually over a period of 240 min from all organs except for bone. Ex vivo autoradiography studies showed selective accumulation in the olfactory tubercles, thalamus, hypothalamus, substantia nigra, superior colliculus, dorsal raphe, and medial raphe as the SERT inhibitors, escitalopram, and IDAM effectively blocked [^18^F]1 localization in these brain regions. PET analysis in rat brains was performed in rats after intravenous injection of 11.1 MBq (0.3 mCi) [^18^F]1. The thalamus, midbrain, and striatum were clearly visualized and peaked at 10–20 min after injection with minimal accumulation in the cerebellum. The thalamus/cerebellum, midbrain/cerebellum, and striatum/cerebellum ratios of 4–4.5 peaked at 100–110 min. Injection of escitalopram and IDAM at 75 min after tracer injection caused a marked drop in radioactivity levels in the thalamus, midbrain, and striatum.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=phenylthio+benzenamine%20and%20%28pig%20or%20cat%20or%20dog%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=phenylthio+benzenamine%20AND%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=phenylthio+benzenamine%20and%20human)]

No publication is currently available.

## NIH Support

MH68782

## References

1 Lucki I. (1998). The spectrum of behaviors influenced by serotonin. Biol Psychiatry.
2 Abi-Dargham A., Laruelle M., Aghajanian G.K., Charney D., Krystal J. (1997). The role of serotonin in the pathophysiology and treatment of schizophrenia. J Neuropsychiatry Clin Neurosci.
3 Charney D.S. (1998). Monoamine dysfunction and the pathophysiology and treatment of depression. J Clin Psychiatry.
4 Parsey R.V., Kegeles L.S., Hwang D.R., Simpson N., Abi-Dargham A., Mawlawi O., Slifstein M., Van Heertum R.L., Mann J.J., Laruelle M. (2000). In vivo quantification of brain serotonin transporters in humans using [11C]McN 5652. J Nucl Med.
5 Szabo Z., Scheffel U., Mathews W.B., Ravert H.T., Szabo K., Kraut M., Palmon S., Ricaurte G.A., Dannals R.F. (1999). Kinetic analysis of [11C]McN5652: a serotonin transporter radioligand. J Cereb Blood Flow Metab.
6 Wilson A.A., Ginovart N., Schmidt M., Meyer J.H., Threlkeld P.G., Houle S. (2000). Novel radiotracers for imaging the serotonin transporter by positron emission tomography: synthesis, radiosynthesis, and in vitro and ex vivo evaluation of (11)C-labeled 2-(phenylthio)araalkylamines. J Med Chem.
7 Houle S., Ginovart N., Hussey D., Meyer J.H., Wilson A.A. (2000). Imaging the serotonin transporter with positron emission tomography: initial human studies with [11C]DAPP and [11C]DASB. Eur J Nucl Med.
8 Wilson A.A., Ginovart N., Hussey D., Meyer J., Houle S. (2002). In vitro and in vivo characterisation of [11C]-DASB: a probe for in vivo measurements of the serotonin transporter by positron emission tomography. Nucl Med Biol.
9 Meyer J.H., Houle S., Sagrati S., Carella A., Hussey D.F., Ginovart N., Goulding V., Kennedy J., Wilson A.A. (2004). Brain serotonin transporter binding potential measured with carbon 11-labeled DASB positron emission tomography: effects of major depressive episodes and severity of dysfunctional attitudes. Arch Gen Psychiatry.
10 Wang J.L., Parhi A.K., Oya S., Lieberman B., Kung M.P., Kung H.F. (2008). 2-(2'-((Dimethylamino)methyl)-4'-(3-[(18)F]fluoropropoxy)-phenylthio)benze namine for positron emission tomography imaging of serotonin transporters. Nucl Med Biol.
11 Parhi A.K., Wang J.L., Oya S., Choi S.R., Kung M.P., Kung H.F. (2007). 2-(2'-((dimethylamino)methyl)-4'-(fluoroalkoxy)-phenylthio)benzenamine derivatives as serotonin transporter imaging agents. J Med Chem.